# [^11^C](+)-4-N-Propyl-,3,4a,5,6,10b-hexahydro-2H-naphth[1,2-b][1,4]-oxazin-9-ol

Chemical name: | [^11^C](+)-4-N-Propyl-,3,4a,5,6,10b-hexahydro-2H-naphth[1,2-b][1,4]-oxazin-9-ol
Abbreviated name: | [^11^C](+)-PHNO
Synonym: | [^11^C](+)-4-Propyl-9-hydroxy-1,2,3,4a,5,6-hexahydronaphthoxazine, [^11^C](+)-4-propyl-9-hydroxynaphthoxazine
Agent Category: | Compound
Target: | Dopamine receptors (D_2_ and D_3_)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PHNO)]

Dopamine, a neurotransmitter, plays an important role in the mediation of movement, cognition, and emotion (1, 2). Dopamine receptors are involved in the pathophysiology of neuropsychiatric diseases, such as Parkinson’s disease, Alzheimer's disease, Huntington’s disease, and schizophrenia (3). Five subtypes of dopamine receptors, D_1_ through D_5_, have been well characterized pharmacologically and biochemically (4). These five subtypes are classified into two subfamilies: D_1_-like (D_1_ and D_5_) and D_2_-like (D_2_, D_3_, and D_4_) dopamine receptors. D_1_-like and D_2_-like receptors exert synergistic as well as opposite effects at both the biochemical and overall system level. A great majority of striatal D_1_ and D_2_ receptors are localized postsynaptically on caudate-putamen neurons and to a lesser extent presynaptically on nigrostriatal axons.

Dopamine receptors are G-protein-coupled receptors and exist in high- and low-affinity states, with respect to agonist binding. The two states are interconvertible. The high-affinity state is coupled to G-proteins, whereas the low-affinity state is not. Dopamine has a dissociation constant (K_d_) of 7 nM for the high-affinity state (K_high_) and a K_d_ of 1,720 nM for the low-affinity state (K_low_) (5). Under physiologic conditions, dopamine is expected to bind predominately to the high-affinity state, which is ~50% occupied by 10 nM dopamine. The high-affinity state has been suggested to be the functional form of the dopamine receptors.

Substituted benzamides, such as sulpiride, raclopride, and iodobenzamide, are specific ligands with only moderate affinity for the D_2_ receptors, making studies of extrastriatal D_2_ receptors difficult (6-8). In binding studies, [^123^I]-labeled epidepride, an analog of isoremoxipride, was found to have high potency and low nonspecific binding, and to be selective for striatal and extrastriatal D_2_ receptors (9). Epidepride has marginal binding to D_4_ receptors, with little affinity for other known neurotransmitter receptors. (S)-N-((1-Allyl-2-pyrrolidinyl)methyl)-5-(3-[^18^F]fluoropropyl)-2,3-dimethoxybenzamide ([^18^F]fallypride), an analog of epidepride, was found to be a selective, high-affinity antagonist of D_2/3_ receptors (10), and in positron emission tomography (PET) in vivo studies (11-13), it identified extrastriatal D_2/3_ receptors. However, none of these antagonists distinguishes between the high- and low-affinity states of the D_2_ receptors. (–)-N-Propyl-norapomorphine (NPA), an agonist of the D_2/3_ receptors, was reported to have K_high_ and K_low_ values of 0.07-0.4 and 20-200 nM, respectively (5, 14, 15). This provides a >50-fold selectivity for the high-affinity over the low-affinity receptors. NPA has good affinity (K_i_ = 0.3 nM) for D_3_ receptors but not other neurotransmitters (16). [^11^C]NPA is being developed as a PET agent for the non-invasive study of the high-affinity state of the D_2/3_ receptors in the brain.

(+)-4-Propyl-3,4,4a,5,6,10b-hexahydro-2H-naphtho[1,2-b][1,4]oxazin-9-ol (PHNO) is an agonist of the D_2_ receptors with a reported K_d_ of 0.56 nM in the canine striatum and a >10,000-fold selectivity for D_2_ over D_1_ receptors (17). PHNO has a high affinity for human cloned D_2_ (K_i_ = 8.5 nM) and D_3_ (K_i_ = 0.16 nM) receptors (18). [^11^C]PHNO showed robust specific binding in the striatum of rodents with insensitivity to displacement by D_1_, norepinephrine, or serotonin ligands (19). [^11^C]PHNO is being developed as a PET agent for the non-invasive study of the high-affinity state of the D_2/3_ receptors in the brain.

.

### Related Resource Links:

- Chapters in MICAD (Dopamine receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=dopamine%20(receptors%20OR%20receptor)+%20AND+Table+AND+micad%5Bbook%5D))
- Gene information in NCBI (D_2_ receptor, (http://www.ncbi.nlm.nih.gov/gene/1813) D_3_ receptor (http://www.ncbi.nlm.nih.gov/gene/1814))
- Articles in Online Mendelian Inheritance in Man (OMIM) (D_2_ receptor (http://www.ncbi.nlm.nih.gov/omim/126450), D_3_ receptor (http://www.ncbi.nlm.nih.gov/omim/126451))
- Clinical trials (Dopamine receptors (http://www.clinicaltrials.gov/ct2/results?term=dopamine+receptor))
- Drug information in Food and Drug Administration (Dopamine receptors (http://google2.fda.gov/search?q=dopamine+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=6&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PHNO%20and%20synthesis)]

Wilson et al. (19) reported a one-pot synthesis of [^11^C]PHNO in which [^11^C]propionyl chloride was reacted with (+)-3,4,4a,5,6,10b-hexahydro-2H-naphtho[1,2-b][1,4]oxazin-9-ol followed by LiAlH_4_ reduction, with an average radiochemical yield of 10% (based on [^11^C]CO_2_, uncorrected, at the end of synthesis). Specific activities were 33-67 GBq/μmol (900-1,800 mCi/μmol at end of synthesis) after high-performance liquid chromatographic purification, with radiochemical purities >99%. [^11^C]Propionyl chloride was prepared by reacting [^11^C]CO_2_ with ethylmagnesium bromide, followed by reaction with phthaloyl chloride. The total synthesis time was 40 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PHNO%20and%20in%20vitro)]

In studies of binding to dopamine receptors in membranes of canine striatum, [^3^H]PHNO had an average K_d_ of 0.56 ± 0.08 nM and a B_max_ of 30.1 ± 2.0 pmol/g tissue (20). Guanilylimidodiphosphate significantly reduced the density of [^3^H]PHNO binding sites, suggesting that [^3^H]PHNO was binding mainly to the high-affinity state of dopamine D_2_ receptors and not to D_3_ receptors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PHNO%20and%20rodentia)]

Biodistribution studies in rats by Wilson et al. (19) showed high accumulation of radioactivity in the striatum (2% of injected dose(ID)/g) within the first 5 min after injection, followed by a gradual decrease of radioactivity to ~0.7% ID/g at 60 min. Accumulation (~1% ID/g) in all other brain regions was similar to that in the cerebellum at 5 min and was only 0.2% ID/g at 60 min. The striatum specific binding ratios (cerebellum as a reference) were 1.1, 2.8, 3.9, and 4.6 at 5, 15, 30, and 60 min after injection, respectively. Haloperidol (D_2_), raclopride (D_2_), PHNO, and RTI-32 (dopamine transporter) pretreatment effectively blocked specific binding of [^11^C]PHNO to the striatum by 73-95%. On the other hand, WAY 100635 (5-HT_1A_), SCH 23390 (D_1_), clonidine (α_2_), and MK-912 (α_2A_) showed little inhibition. Amphetamine (a dopamine releaser) pretreatment revealed dose-dependent inhibition of [^11^C]PHNO binding to the striatum, indicating that [^11^C]PHNO binding is sensitive to endogenous dopamine levels in the striatum. At 40 min post injection, 26% of [^11^C]PHNO radioactivity remained intact in the plasma, with 74% as polar metabolites. However, >98% of the radioactivity in the rat brain was intact [^11^C]PHNO, suggesting that the polar metabolites cannot cross the blood-brain barrier. [^11^C]PHNO thus displays uptake and washout kinetics characteristic of reversible radiotracers as well as excellent selectivity toward D_2/3_ receptors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PHNO%20and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

Ginovart et al. (21) reported on [^11^C]PHNO PET study in cats. [^11^C]PHNO displayed high uptake in the striatum with a mean striatal binding potential (BP) of 3.95 ± 0.85. Pretreatment with the specific antagonists SCH 23390 (D_1_ antagonist), raclopride (D_2_ antagonist), haloperidol (D_2_ antagonist), and SB-277011 (D_3_ antagonist) indicated that [^11^C]PHNO binding in the striatum is specific to D_2_ receptors because raclopride and haloperidol showed >89% inhibition, whereas SCH 23390 and SB-277011 showed no inhibition. The BP of [^11^C]PHNO in the striatum was 2.5-fold higher than that measured with [^11^C]NPA. The BP of [^11^C]raclopride was reduced by 13, 39, and 57% after amphetamine doses of 0.1, 0.5, and 2.0 mg/kg, respectively. The BP of [^11^C]PHNO was reduced by 21, 67, and 83% after amphetamine doses of 0.1, 0.5, and 2.0 mg/kg, respectively. Amphetamine induced up to 83 ± 4% inhibition of the [^11^C]PHNO BP, but only up to 57 ± 8% inhibition of the [^11^C]raclopride BP. Thus, [^11^C]PHNO was more sensitive to the dopamine-releasing effect of amphetamine than [^11^C]raclopride. Because raclopride binds to receptors in both the high- and low-affinity states and dopamine binds with high affinity mainly to receptors in the high-affinity state, the percentage reduction is greater when an agonist is used than when an antagonist is used. This large proportion of high-affinity sites might explain the vulnerability of D_2_ radiotracers to competition by endogenous dopamine and is consistent with the reported in vivo binding of the agonist radiotracer [^11^C]PHNO. Scatchard analyses of [^11^C]PHNO and [^11^C]raclopride binding in two cats revealed that the B_max_ values obtained with the agonist (29.6 and 32.9 pmol/ml) were similar to those obtained with the antagonist (30.6 and 33.4 pmol/ml).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PHNO%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PHNO%20and%20human)]

Willeit et al. (22) performed preliminary PET studies of two male and two female healthy volunteers with [^11^C]PHNO under baseline conditions and after haloperidol pretreatment. The simplified reference tissue method of Lammertsma and Hume (23) was used to derive BPs for each region of interest. The [^11^C]PHNO BPs in the caudate, putamen, and globus pallidus were 3.00 ± 0.4, 3.10 ± 0.2, and 4.17 ± 1.2, respectively. Small but detectable binding was identified in the substantia nigra/ventral tegmental area. Preliminary test-retest data in two subjects suggested that the BP estimates were reliable. Pretreatment of two subjects with haloperidol (2 mg) reduced the BPs in the caudate, putamen, and globus pallidus by 14-49% with no detectable changes in the cerebellum. [^11^C]Raclopride binding was studied in two of the subjects. The [^11^C]raclopride BPs in the caudate, putamen, and globus pallidus were 3.3 ± 0.7, 4.1 ± 0.4, and 1.4 ± 0.2, respectively. [^11^C]PHNO binding compared with [^11^C]raclopride binding was lower in the caudate (–8.8%) and putamen (–23.5%) but higher in the globus pallidus (+200%). [^11^C]PHNO showed favorable kinetics and may allow reliable quantitation of high-affinity D_2/3_ receptors in the brain.

## References

1 Carbon M., Ghilardi M.F., Feigin A., Fukuda M., Silvestri G., Mentis M.J., Ghez C., Moeller J.R., Eidelberg D. (2003). Learning networks in health and Parkinson's disease: reproducibility and treatment effects. Hum Brain Mapp.
2 Chesselet M.F., Delfs J.M. (1996). Basal ganglia and movement disorders: an update. Trends Neurosci.
3 Seeman P., Bzowej N.H., Guan H.C., Bergeron C., Reynolds G.P., Bird E.D., Riederer P., Jellinger K., Tourtellotte W.W. (1987). Human brain D1 and D2 dopamine receptors in schizophrenia, Alzheimer's, Parkinson's, and Huntington's diseases. Neuropsychopharmacology.
4 Stoof J.C., Kebabian J.W. (1984). Two dopamine receptors: biochemistry, physiology and pharmacology. Life Sci.
5 George S.R., Watanabe M., Di Paolo T., Falardeau P., Labrie F., Seeman P. (1985). The functional state of the dopamine receptor in the anterior pituitary is in the high affinity form. Endocrinology.
6 Gehlert D.R., Wamsley J.K. (1984). Autoradiographic localization of [3H]sulpiride binding sites in the rat brain. Eur J Pharmacol.
7 Lidow M.S., Goldman-Rakic P.S., Rakic P., Innis R.B. (1989). Dopamine D2 receptors in the cerebral cortex: distribution and pharmacological characterization with [3H]raclopride. Proc Natl Acad Sci U S A.
8 Brucke T., Tsai Y.F., McLellan C., Singhanyom W., Kung H.F., Cohen R.M., Chiueh C.C. (1988). In vitro binding properties and autoradiographic imaging of 3-iodobenzamide ([125I]-IBZM): a potential imaging ligand for D-2 dopamine receptors in SPECT. Life Sci.
9 Kessler R.M., Ansari M.S., Schmidt D.E., de Paulis T., Clanton J.A., Innis R., al-Tikriti M., Manning R.G., Gillespie D. (1991). High affinity dopamine D2 receptor radioligands. 2. [125I]epidepride, a potent and specific radioligand for the characterization of striatal and extrastriatal dopamine D2 receptors. Life Sci.
10 Mukherjee J., Yang Z.Y., Das M.K., Brown T. (1995). Fluorinated benzamide neuroleptics--III. Development of (S)-N-[(1-allyl-2-pyrrolidinyl)methyl]-5-(3-[18F]fluoropropyl)-2, 3-dimethoxybenzamide as an improved dopamine D-2 receptor tracer. Nucl Med Biol.
11 Grunder G., Landvogt C., Vernaleken I., Buchholz H.G., Ondracek J., Siessmeier T., Hartter S., Schreckenberger M., Stoeter P., Hiemke C., Rosch F., Wong D.F., Bartenstein P. (2006). The striatal and extrastriatal D2/D3 receptor-binding profile of clozapine in patients with schizophrenia. Neuropsychopharmacology.
12 Mukherjee J., Christian B.T., Narayanan T.K., Shi B., Collins D. (2005). Measurement of d-amphetamine-induced effects on the binding of dopamine D-2/D-3 receptor radioligand, 18F-fallypride in extrastriatal brain regions in non-human primates using PET. Brain Res.
13 Riccardi P., Li R., Ansari M.S., Zald D., Park S., Dawant B., Anderson S., Doop M., Woodward N., Schoenberg E., Schmidt D., Baldwin R., Kessler R. (2006). Amphetamine-induced displacement of [18F] fallypride in striatum and extrastriatal regions in humans. Neuropsychopharmacology.
14 Gardner B., Strange P.G. (1998). Agonist action at D2(long) dopamine receptors: ligand binding and functional assays. Br J Pharmacol.
15 Lahti R.A., Mutin A., Cochrane E.V., Tepper P.G., Dijkstra D., Wikstrom H., Tamminga C.A. (1996). Affinities and intrinsic activities of dopamine receptor agonists for the hD21 and hD4.4 receptors. Eur J Pharmacol.
16 Neumeyer J.L., Neustadt B.R., Oh K.H., Weinhardt K.K., Boyce C.B., Rosenberg F.J., Teiger D.G. (1973). Aporphines. 8. Total synthesis and pharmacological evaluation of (plus or minus)-apomorphine, (plus or minus)-apocodeine, (plus or minus)-N-n-propylnorapomorphine, and (plus or minus)-N-n-propylnorapocodeine. J Med Chem.
17 Seeman P., Ulpian C., Larsen R.D., Anderson P.S. (1993). Dopamine receptors labelled by PHNO. Synapse.
18 Freedman S.B., Patel S., Marwood R., Emms F., Seabrook G.R., Knowles M.R., McAllister G. (1994). Expression and pharmacological characterization of the human D3 dopamine receptor. J Pharmacol Exp Ther.
19 Wilson A.A., McCormick P., Kapur S., Willeit M., Garcia A., Hussey D., Houle S., Seeman P., Ginovart N. (2005). Radiosynthesis and evaluation of [11C]-(+)-4-propyl-3,4,4a,5,6,10b-hexahydro-2H-naphtho[1,2-b][1,4]oxazin-9 -ol as a potential radiotracer for in vivo imaging of the dopamine D2 high-affinity state with positron emission tomography. J Med Chem.
20 Nobrega J.N., Seeman P. (1994). Dopamine D2 receptors mapped in rat brain with [3H](+)PHNO. Synapse.
21 Ginovart N., Galineau L., Willeit M., Mizrahi R., Bloomfield P.M., Seeman P., Houle S., Kapur S., Wilson A.A. (2006). Binding characteristics and sensitivity to endogenous dopamine of [C]-(+)-PHNO, a new agonist radiotracer for imaging the high-affinity state of D receptors in vivo using positron emission tomography. J Neurochem.
22 Willeit M., Ginovart N., Kapur S., Houle S., Hussey D., Seeman P., Wilson A.A. (2006). High-affinity states of human brain dopamine D2/3 receptors imaged by the agonist [11C]-(+)-PHNO. Biol Psychiatry.
23 Lammertsma A.A., Hume S.P. (1996). Simplified reference tissue model for PET receptor studies. Neuroimage.